# ^111^In-2-(p-isothiocyanatobenzyl)-6-methyl-diethylenetriamine-N,N,N´,N´´,N´´-pentaacetic acid-trastuzumab

Chemical name: | ^111^In-2-(p-isothiocyanatobenzyl)-6-methyl-diethylenetriamine-N,N,N´,N´´,N´´-pentaacetic acid-trastuzumab
Abbreviated name: | ^111^In-1B4M-DTPA-humAb4D5-8
Synonym: | ^111^In-Herceptin^®^, ^111^In-anti-HER2 MAb
Agent Category: | Antibody
Target: | Human epidermal growth factor receptor 2 (HER2)
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=119533), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=183984) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-trastuzumab%20OR%20111In-Herceptin%29)]

^111^In-2-(p-isothiocyanatobenzyl)-6-methyl-diethylenetriamine-N,N,N´,N´´,N´´-pentaacetic acid-trastuzumab (^111^In-1B4M-DTPA-humAb4D5-8), which is formed by the conjugation of ^111^In with an intact recombinant humanized monoclonal antibody (MAb) against the antigen of human epidermal growth factor receptor 2 (HER2), has been developed for imaging of human breast cancer (1). ^111^In is a gamma emitter with a physical half-life (t_½_) of 2.8 days.

The epidermal growth factor receptors (HER/erbB) with tyrosine kinase activity are involved in transmission of signals controlling normal cell development, growth, differentiation, and survival (2-4). This cell-surface receptor family consists of four distinct members, the epidermal growth factor receptors HER1, HER2, HER3, and HER4. These receptors are found in various combinations in different tissues. There are nine ligands that bind directly to HER1, HER3, or HER4. HER2 can be activated as a result of ligand binding to other HER receptors. The ligandless HER2 receptor is encoded by the human gene HER2/c-erbB2 (HER2/neu). It has been found to be overexpressed in a wide variety of human cancers and in 20-30% of primary breast cancers (5). This overexpression is associated with aggressive tumor growth and metastatic activity. In breast cancer, HER2/neu gene amplification can result in 10- to 100-fold higher HER2 protein levels in tumor cells than that in normal breast epithelium. HER2 overexpression is considered a negative prognostic indicator for breast cancer.

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (6-8). Anti-HER2 MAbs have been generated for inhibiting the growth of tumor cells that possess activated HER2/neu receptors (9). Murine 4D5 MAb was raised against human breast and ovarian tumor cell lines overexpressing p185^HER2^. This MAb was found to recognize an extracellular epitope (amino acids 529 to 627) in the cysteine-rich II domain that resides very close to the transmembrane region (9). Murine 4D5 MAb was fully humanized by Carter et al. (10) to generate the humAb4D5-8 MAb in an effort to improve the safety and tolerance of the antibody for clinical applications. Trastuzumab is of the IgG_1_ kappa class and binds to the recombinant HER2 extracellular domain with an affinity constant (K_d_) of 0.1 nM. Trastuzumab is approved by the Food and Drug Administration to treat breast cancer that is HER2 positive and has metastasized to other areas of the body. It has also been studied in the treatment of other types of cancer. Cardiotoxicity is the most serious complication of using trastuzumab in humans (5, 11). One potential application of a radiolabeled anti-HER2 MAb is the pretreatment imaging of breast cancer patients to predict the cardiotoxicity and therapeutic efficacy of unlabeled trastuzumab.

Various anti-HER2 MAbs have been labeled with ^131^I, ^125^I, ^111^In, ^86^Y, ^90^Y, ^64^Cu, ^76^Br, or Gd for potential imaging and therapeutic applications (1, 12-18). The labeling with radiometals is generally achieved by indirect labeling with use of a bifunctional chelating agent (19, 20). ^111^In, a photon emitter with a physical half-life (t_½_) of 2.8 days, is considered one of the radionuclides of choice for antibody imaging studies.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28111In%5BAll%20Fields%5D%20AND%20%28%22trastuzumab%22%5BSubstance%20Name%5D%20OR%20Trastuzumab%5BText%20Word%5D%29%29%20OR%20111In-Herceptin%5BAll%20Fields%5D%29%20AND)]

Trastuzumab was synthesized by humanization of murine 4D5 MAb (10). In this procedure, the complementarity-determining regions of the murine 4D5 MAb were transplanted into a human antibody model. A “gene conversion mutagenesis” strategy was used to simultaneously humanize the heavy- and light-chain region genes. A final “humanized” antibody, humAb4D5, containing only the antigen-binding loops from murine 4D5 MAb and human variable region framework residues plus IgG_1_ constant domains, was constructed. Of 8 humanized variants, humAb4D5-8 was found to bind its antigen 3-fold more tightly than the murine 4D5 MAb.

Garmestani et al. (1) used a bifunctional ligand, 2-(p-isothiocyanatobenzyl)-6-methyl-diethylenetriamine-N,N,N´,N´´,N´´-pentaacetic acid (1B4M-DTPA), for the antibody conjugation. The ligand was synthesized as described by Brechbiel et al. (21). Briefly, penta-tert-butyl ester was prepared from diethylenetriamine trihydrochloride by alkylation with tert-butyl bromoacetate with bisodium carbonate in dimethylformamide. The obtained product was then treated with trifluoroacetic acid for 18 h. The ligand was purified by chromatography. The yield of IB4M-DTPA from the triamine was 30-36%. Conjugation was performed as reported by Kozak et al. (22). In the radiolabeling procedures, the 1B4M-DTPA-humAb4D5-8 conjugate in 0.15 M ammonium acetate buffer was added to 74 MBq (2 mCi) ^111^In (pH = 5.5-6.0). The reaction mixture was incubated at 37°C for 30 min. The reaction was quenched by adding 0.05 M ethylenediaminetetraacetatic acid to scavenge any unlabeled ^111^In. The ^111^In-1B4M-DTPA-humAb4D5-8 was purified by size exclusion high-performance liquid chromatography. The radiolabeling efficiency was 73 ± 3%, and the specific activity of ^111^In-1B4M-DTPA-humAb4D5-8 was reported to be 70.3 MBq (1.9 mCi)/mg (10.64 GBq (0.29 Ci)/µmol). Kobayashi et al. (18) used the same bifunctional chelator for radiolabeling by reacting humAb4D5 with a 20-fold molar excess of 1B4M-DTPA to produce 1B4M-DTPA-humAb4D5-8. The immunoconjugate was then reacted with ^111^InCl_3_ in 0.3 M sodium acetate buffer at pH 6.0 for 15 min at room temperature.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20in%20vitro)]

The immunoreactivity of ^111^In-1B4M-DTPA-humAb4D5-8 was assessed in a live-cell radioimmunoassay with HER2-positive N87 (human gastric carcinoma) cells (1). The percentage binding was 45.8%. Kobayashi et al. (18) reported that the maximum binding of ^111^In-1B4M-DTPA-humAb4D5-8 to WIBC-9 inflammatory breast cancer cells was 82%. Ninety-five percent of the binding was inhibited by the addition of nonradiolabeled humAb4D5-8..

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20rodentia)]

Garmestani et al. (1) reported the biodistribution of ^111^In-1B4M-DTPA-humAb4D5-8 (185 kBq (5 µCi); n = 5) in mice bearing s.c. HER2-positive LS-174T tumors (tumor diameter, 0.4-0.6 cm). The tumor radioactivity uptakes (% ID/g) were 29.72 ± 9.68, 38.20 ± 11.66, 63.51 ± 19.77, 66.86 ± 10.96, and 24.17 ± 17.63 at 12, 24, 48, 72, and 120 h after injection, respectively. The radiolocalization indices (tumor % ID/g divided by the femur % ID/g) were 11.3 ± 6.95, 18.9 ± 5.63, 37.2 ± 13.59, 37.9 ± 10.81, and 25.3 ± 17.23 at 12, 24, 48, 72, and 120 h, respectively. The blood radioactivities (% ID/g) were 19.56 ± 1.72, 16.08 ± 1.52, 14.04 ± 3.76, 13.12 ± 0.41, and 7.09 ± 2.82 at 12, 24, 48, 72, and 120 h, respectively. The blood clearance half-lives (t_½α_ and t_½β_) were 2.67 and 91.9 h, respectively. The 24-h % ID/g values were 5.19 ± 0.63, 4.48 ± 0.61, 6.74 ± 3.02, 6.14 ± 0.52, and 4.13 ± 0.44 for the liver, spleen, kidney, lung, and heart, respectively. No specific blocking study was reported. Using mice bearing HER2-positive WIBC-9 tumors, Kobayashi et al. (18) showed that the maximum tumor uptake of ^111^In-1B4M-DTPA-humAb4D5-8 (29.6 kBq (0.8 μCi) i.v.) at 24 h was ~30% ID/g (extracted from Figure 1 of Kobayashi et al. (18), n = 4-5). The liver radioactivity uptake was ~5% ID/g at 24 h (extracted from Figure 1 of Kobayashi et al. (18)). Lub-de Hooge et al. (4) suggested that ^111^In-1B4M-DTPA-humAb4D5-8 had lower liver uptake but more prolonged blood pool activity than ^111^In-DTPA-humAb4D5-8.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIH Intramural Support.

## References

1 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
2 Frankel C. Development and clinical overview of trastuzumab (herceptin) Semin Oncol Nurs 2000 16Suppl 14 13 7 11151453
3 Sliwkowski M.X. Lofgren J.A. Lewis G.D. Hotaling T.E. Fendly B.M. Fox J.A. Nonclinical studies addressing the mechanism of action of trastuzumab (Herceptin) Semin Oncol 1999 26Suppl 124 60 70 10482195
4 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
5 Slamon D.J., Leyland-Jones B., Shak S., Fuchs H., Paton V., Bajamonde A., Fleming T., Eiermann W., Wolter J., Pegram M., Baselga J., Norton L. (2001). Use of chemotherapy plus a monoclonal antibody against HER2 for metastatic breast cancer that overexpresses HER2. N Engl J Med.
6 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
7 Milenic D.E., Brechbiel M.W. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
8 Kowalsky R.J., Falen S.W. (2004). Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. , Washington, D.C.: APhA. 733-752.
9 Fendly B.M., Winget M., Hudziak R.M., Lipari M.T., Napier M.A., Ullrich A. (1990). Characterization of murine monoclonal antibodies reactive to either the human epidermal growth factor receptor or HER2/neu gene product. Cancer Res.
10 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
11 Behr T.M., Behe M., Wormann B. (2001). Trastuzumab and breast cancer. N Engl J Med.
12 Blend M.J., Stastny J.J., Swanson S.M., Brechbiel M.W. (2003). Labeling anti-HER2/neu monoclonal antibodies with 111In and 90Y using a bifunctional DTPA chelating agent. Cancer Biother Radiopharm.
13 Olafsen T., Kenanova V.E., Sundaresan G., Anderson A.L., Crow D., Yazaki P.J., Li L., Press M.F., Gambhir S.S., Williams L.E., Wong J.Y., Raubitschek A.A., Shively J.E., Wu A.M. (2005). Optimizing radiolabeled engineered anti-p185HER2 antibody fragments for in vivo imaging. Cancer Res.
14 Winberg K.J., Persson M., Malmstrom P.U., Sjoberg S., Tolmachev V. (2004). Radiobromination of anti-HER2/neu/ErbB-2 monoclonal antibody using the p-isothiocyanatobenzene derivative of the [76Br]undecahydro-bromo-7,8-dicarba-nido-undecaborate(1-) ion. Nucl Med Biol.
15 Xu F.J., Yu Y.H., Bae D.S., Zhao X.G., Slade S.K., Boyer C.M., Bast R.C., Zalutsky M.R. (1997). Radioiodinated antibody targeting of the HER-2/neu oncoprotein. Nucl Med Biol.
16 Palm S., Enmon R.M., Matei C., Kolbert K.S., Xu S., Zanzonico P.B., Finn R.L., Koutcher J.A., Larson S.M., Sgouros G. (2003). Pharmacokinetics and Biodistribution of (86)Y-Trastuzumab for (90)Y dosimetry in an ovarian carcinoma model: correlative MicroPET and MRI. J Nucl Med.
17 Tsai S.W., Sun Y., Williams L.E., Raubitschek A.A., Wu A.M., Shively J.E. (2000). Biodistribution and radioimmunotherapy of human breast cancer xenografts with radiometal-labeled DOTA conjugated anti-HER2/neu antibody 4D5. Bioconjug Chem.
18 Kobayashi H., Shirakawa K., Kawamoto S., Saga T., Sato N., Hiraga A., Watanabe I., Heike Y., Togashi K., Konishi J., Brechbiel M.W., Wakasugi H. (2002). Rapid accumulation and internalization of radiolabeled herceptin in an inflammatory breast cancer xenograft with vasculogenic mimicry predicted by the contrast-enhanced dynamic MRI with the macromolecular contrast agent G6-(1B4M-Gd)(256). Cancer Res.
19 Fritzberg A.R., Berninger R.W., Hadley S.W., Wester D.W. (1988). Approaches to radiolabeling of antibodies for diagnosis and therapy of cancer. Pharm Res.
20 Hnatowich D.J., Childs R.L., Lanteigne D., Najafi A. (1983). The preparation of DTPA-coupled antibodies radiolabeled with metallic radionuclides: an improved method. J Immunol Methods.
21 Brechbiel M.W., Beitzel P.M., Gansow O.A. (1997). Purification of p-nitrobenzyl C-functionalized diethylenetriamine pentaacetic acids for clinical applications using anion-exchange chromatography. J Chromatogr A.
22 Kozak R.W., Raubitschek A., Mirzadeh S., Brechbiel M.W., Junghans R.P., Gansow O.A., Waldmann T.A. (1989). Nature of the bifunctional chelating agent used for radioimmunotherapy with yttrium-90 monoclonal antibodies: critical factors in determining in vivo survival and organ toxicity. Cancer Res.